# ^64^Cu-Labeled 1,4,7-tris(acetic acid)-10-vinylsulfone-1,4,7,10-tetraazacyclododecane conjugated to Cys^40^-Exendin-4

Chemical name: | ^64^Cu-Labeled 1,4,7-tris(acetic acid)-10-vinylsulfone-1,4,7,10-tetraazacyclododecane conjugated to Cys^40^-Exendin-4
Abbreviated name: | ^64^Cu-DO3A-VS-Cys^40^-Exendin-4
Synonym:
Agent Category: | Ligand
Target: | Glucagon-like peptide 1 receptor (GLP-1R)
Target Category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^64^Cu
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Glucagon-like%20peptide%201%20receptor&cmd=DetailsSearch)]

A characteristic clinical feature of diabetes, an autoimmune disease, is diminished secretion and/or function of insulin and little or no glycemic control (1-3). The onset of diabetes is a complex process, and the pathophysiology of this disease is not completely understood (4). Diabetes has been classified into two types: Type 1 (http://www.diabetes.org/diabetes-basics/type-1/) (T1D) and Type 2 (http://www.diabetes.org/diabetes-basics/type-2/) (T2D). Among these, T1D is the chronic form of the disorder and is usually triggered by environmental factors in young people (<30 years of age) who are genetically predisposed to it; however, some individuals >30 years of age may also develop T1D (5). T1D is also known as juvenile-onset diabetes. People develop T2D because their muscles and adipose tissue are resistant to insulin, and it usually manifests in older (>50 years of age) and/or obese individuals (5). Although exercise and diet can alleviate this disorder to some extent, the blood glucose levels of individuals who suffer from diabetes have to be monitored several times a day or on a regular basis (weekly or monthly). Drugs (such as recombinant insulin (http://www.lantus.com/learn/default.aspx?WT.mc_id=LNWB1557&WT.srch=1)) that are available to treat diabetes must be used lifelong after diagnosis, and a treatment(s) that can effectively prevent the disease is not yet available (6).

In humans, insulin is produced by the β cells that are located in the islets of Langerhans of the pancreas. Approximately 80% of the islet cells are composed of the β cells, and reduced or the absence of function of these cells (due to T-cell–mediated destruction) in individuals with diabetes leads to low or a complete lack of insulin secretion. Transplantation of islet cells is considered to be the most suitable treatment for diabetes, but only 10%–15% of the patients who undergo this procedure remain insulin-independent beyond 5 years. Reasons for the loss of the grafted islet cell functions are not completely understood (7). Currently, only indirect methods are used to monitor the functioning of the transplanted islet cells, and usually by the time the loss in function is apparent it is too late to rescue the transplanted islets. In addition, noninvasive imaging probes that have been evaluated to monitor the β cells produced suboptimal results, and agents that may produce accurate images of the transplanted cells are still under development (1, 7).

The β cells have a high expression of the glucagon-like peptide 1 (GLP-1) receptor (GLP-1R), and the GLP-1R ligand (on binding to the receptor it enhances insulin secretion from the β cells) can be a suitable probe for the visualization of these cells in the pancreas. A major limitation of using this peptide for imaging purposes is its rapid degradation under physiological conditions (1). Exendin-4, a peptide hormone isolated from the saliva of the gila monster, has properties similar to those of GLP-1, is more stable than GLP-1 in vivo, and has a high affinity for the GLP-1R (1). Previously, investigators labeled derivatives of Exendin-4 with radionuclides such as 111In, 125I, 68Ga, etc., and used the probes with single-photon emission computed tomography (SPECT) to visualize GLP-1R–positive insulinomas (http://www.cancer.gov/dictionary?CdrID=657853) in preclinical studies (1) and in humans (8, 9). However, positron emission tomography (PET) imaging is known to have a higher resolution and sensitivity compared to SPECT and can be used to accurately investigate various biological processes in living systems. Wu et al. developed a ^64^Cu-labeled Exendin analog (^64^Cu-labeled 1,4,7-tris(acetic acid)-10-vinylsulfone-1,4,7,10-tetraazacyclododecane (DO3A) conjugated to Cys^40^-Exendin-4 (^64^Cu-DO3A-VS-Cys^40^-Exendin-4)) and investigated its biodistribution in mice bearing subcutaneous INS-1 cell tumors (a rat insulinoma cell line that overexpresses GLP-1R) (1). The probe was also evaluated for the PET visualization of INS-1 cell xenograft tumors and islet cells transplanted into the liver of the animals.

### Related Resource Links

Human GLP-1R Protein (http://www.ncbi.nlm.nih.gov/protein/CAB71177.1) and mRNA (http://www.ncbi.nlm.nih.gov/nuccore/NM_002062.3) sequences

Clinical trials (http://clinicaltrials.gov/ct2/results?term=Glucagon-like+peptide+1+receptor) involving GLP-1R

GLP-1R antagonists in clinical trials (http://clinicaltrials.gov/ct2/results?term=Glucagon-like+peptide+1+receptor+antagonists)

GLP-1R in Online Mendelian Inheritance in Man Database (http://omim.org/entry/138032) (OMIM)

Medications (http://www.drugs.com/condition/diabetes-mellitus-type-i.html) for diabetes, Type 1

Medications (http://www.drugs.com/condition/diabetes-mellitus-type-ii.html) for Type 2 diabetes

Genome-Wide Association Studies: Diabetes Type 1 (http://www.ncbi.nlm.nih.gov/pubmed?term=Genome%20wide%20association%20studies%20for%20Type%201%20diabetes)

Genome-Wide Association Studies: Diabetes Type 2 (http://www.ncbi.nlm.nih.gov/pubmed?term=Genome%20wide%20association%20studies%20for%20Type%202%20diabetes)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=21692471%5Buid%5D&cmd=DetailsSearch)]

The synthesis of DO3A-VS-Cys^40^-Exendin-4 and its labeling with ^64^Cu have been described in detail by Wu et al. (1). The radiochemical yield and purity of the labeled compound were reported to be >95% (n = 5 reactions) and >99%, respectively. The specific activity of ^64^Cu-DO3A-VS-Cys^40^-Exendin-4 was ~2.4 GBq/mol (~89 Ci/mol).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%2864%29Cu-DO3A-VS-Cys%2840%29-Exendin-4%20in%20vitro&cmd=DetailsSearch)]

Using a competitive binding assay of ^125^I-Exendin(9-39) with INS-1 cells, the IC_50_ values of DO3A-VS-Cys^40^-Exendin-4 (without Cu) and Exendin-4 were determined to be 190.6 ± 3.5 pM and 131.07 ± 8.3 pM, respectively (1). This indicated that the conjugation of DO3A had little effect on the receptor binding affinity of the Exendin-4 derivative.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=21692471%5Buid%5D&cmd=DetailsSearch)]

The biodistribution of ^64^Cu-DO3A-VS-Cys^40^-Exendin-4 was investigated in non-obese diabetic/severe combined immunodeficient (NOD/SCID) mice (n = 3 animals/time point) bearing INS-1 cell xenograft tumors on the left flank as described by Wu et al. (1). The mice were injected with 0.37 MBq ^64^Cu-DO3A-VS-Cys^40^-Exendin-4 (0.05 μg in 100 μL) through the tail vein, and the animals were euthanized at preselected time points to quantify the amount of radioactivity accumulated in the various organs of interest. Data from this study were presented as percent injected dose per gram tissue (% ID/g). The uptake of radioactivity in the tumors was 12.7 ± 2.9% ID/g, 14.2 ± 2.6% ID/g, and 9.2 ± 4.0% ID/g at 1, 4, and 23 h postinjection (p.i.), respectively. Accumulation values of the label in the lung and pancreas (both these organs have a high expression of GLP-1R) were between ~7.5% ID/g (at 1 h p.i.) and ~4% ID/g (at 2 h and 23 h p.i.). Maximum uptake was observed in the kidneys (46.8 ± 11.4% ID/g at 23 h p.i.), indicating that the radiolabeled compound was excreted through the urinary route.

The receptor binding specificity of ^64^Cu-DO3A-VS-Cys^40^-Exendin-4 was investigated in a blocking experiment (1). For this, the NOD/SCID mice (n = 3 animals) were injected with the labeled compound in the presence of excess (~4.8 nmol) unlabeled Exendin-4, and the animals were euthanized at 4 h p.i. to determine the amount of radioactivity present in the various organs, including the tumors. The amount of label in the tumors of these animals was significantly lower (2.7 ± 2.0% ID/g; P < 0.01) than in the tumors of animals injected with ^64^Cu-DO3A-VS-Cys^40^-Exendin-4 without unlabeled exendin-4 (14.2 ± 2.6% ID/g). Similarly, in the blocking study, the GLP-1R–positive organs (lung and pancreas) were reported to have a significantly reduced up take of radioactivity.

MicroPET images of NOD/SCID mice (n = 3 animals/time point) bearing INS-1 cell xenograft tumors were acquired at 1, 4, and 22 h after an intravenous injection of ^64^Cu-DO3A-VS-Cys^40^-Exendin-4 through the tail vein (1). The tumors were clearly visible in the images, with a high tumor/background ratio at all the time points, and no tumor was visible in the PET images of animals used for the blocking experiment. This indicated that ^64^Cu-DO3A-VS-Cys^40^-Exendin-4 bound specifically to GLP-1R expressed by the INS-1 cell xenograft tumors.

In another study to test the probe in an islet transplant model, human islet cells were transplanted into the livers of NOD/SCID mice (n = 3 animals/time point; number of cells transplanted not reported) through the portal vein (1). Control animals had no islet cell transplants. Nine days after implantation, the animals were injected with 3.7–7.4 MBq (0.1–0.2 mCi) ^64^Cu-DO3A-VS-Cys^40^-Exendin-4, and microPET images of the animals were acquired at 2 h and 5 h p.i. Wu et al. converted image intensities to % ID/g (1). The amount of tracer in the liver of the transplant animals was significantly higher (4.0 ± 0.2% ID/g and 5.3 ± 0.7% ID/g at 2 h and 5 h p.i., respectively; P < 0.01) than in the liver of the control animals (1.7 ± 0.6% ID/g and 2.4 ± 0.8% ID/g at 2 h and 5 h p.i., respectively). Presence of the human islet cells in the mouse liver and the expression of GLP-1R by the islets (similar to the islet cells in the human pancreas) have been confirmed with histology as detailed elsewhere (1).

From these studies, the investigators concluded that ^64^Cu-DO3A-VS-Cys^40^-Exendin-4 is a suitable PET agent for the imaging of insulinoma tumors and human islet cells transplanted intraportally in mice (1).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=21692471%5Buid%5D&cmd=DetailsSearch)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=21692471%5Buid%5D&cmd=DetailsSearch)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=21692471%5Buid%5D&cmd=DetailsSearch)]

No publication is currently available.

## Supplemental Information

[Disclaimers]

No supplemental information is currently available.

## References

1 Wu Z., Todorov I., Li L., Bading J.R., Li Z., Nair I., Ishiyama K., Colcher D., Conti P.E., Fraser S.E., Shively J.E., Kandeel F. (2011). In Vivo Imaging of Transplanted Islets with (64)Cu-DO3A-VS-Cys(40)-Exendin-4 by Targeting GLP-1 Receptor. Bioconjug Chem.
2 Gallwitz, B., C. Kazda, P. Kraus, C. Nicolay, and G. Schernthaner, Contribution of insulin deficiency and insulin resistance to the development of type 2 diabetes: nature of early stage diabetes. Acta Diabetol, 2011
3 Waldron-Lynch F., Herold K.C. (2011). Immunomodulatory therapy to preserve pancreatic beta-cell function in type 1 diabetes. Nat Rev Drug Discov.
4 Guay C., Roggli E., Nesca V., Jacovetti C., Regazzi R. (2011). Diabetes mellitus, a microRNA-related disease?. Transl Res.
5 van Belle T.L., Coppieters K.T., von Herrath M.G. (2011). Type 1 diabetes: etiology, immunology, and therapeutic strategies. Physiol Rev.
6 Thrower S.L., Bingley P.J. (2009). Strategies to prevent type 1 diabetes. Diabetes Obes Metab.
7 Borot, S., L.A. Crowe, C. Toso, J.P. Vallee, and T. Berney, Noninvasive Imaging Techniques in Islet Transplantation. Curr Diab Rep, 2011
8 Christ E., Wild D., Forrer F., Brandle M., Sahli R., Clerici T., Gloor B., Martius F., Maecke H., Reubi J.C. (2009). Glucagon-like peptide-1 receptor imaging for localization of insulinomas. J Clin Endocrinol Metab.
9 Wild D., Macke H., Christ E., Gloor B., Reubi J.C. (2008). Glucagon-like peptide 1-receptor scans to localize occult insulinomas. N Engl J Med.